# ^111^In-Labeled multifunctional single-attachment-point reagent-c[RGDfK]

Chemical name: | ^111^In-Labeled multifunctional single-attachment-point reagent-c[RGDfK] | [image]
Abbreviated name: | ^111^In-MSAP-RGD | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Integrin α_v_β_3_ | [image]
Target Category: | Receptors | [image]
Method of detection: | Multimodality imaging (SPECT and optical imaging) | [image]
Source of signal / contrast: | ^111^In and Cy5.5 | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^111^In-MSAP-RGD (1)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=molecular%20imaging%20and%20integrin%20%CE%B1v%CE%B23)]

^111^In-Labeled multifunctional single-attachment-point reagent (MSAP)-c[RGDfK], abbreviated as ^111^In-MSAP-RGD, is a multimodality imaging agent synthesized by Bunschoten et al. for imaging tumors by targeting integrin α_v_β_3_ (1). MSAP is a conjugate that consists of a Cy5.5 derivative (CyAL-5.5b) and a chelate of diethylenetriamine pentaacetic acid (DTPA). CyAL-5.5b is a symmetric, monofunctional pentamethine carbocyanine fluorophore with an alkyl carboxylic acid functional group (λ_ex_ = 674 nm, λ_em_ = 693 nm).

Angiogenesis is a process of neovascular development and growth from pre-existing vessels. Unlike the normal blood vessel system, the neovasculature is chaotic and irregular in tumors with abnormal expression of diverse vascular surface biomarkers. These biomarkers have fewer kinetic compartments that must be crossed for intravenously administered agents to reach them (2, 3). Integrin α_v_β_3_ is one of these biomarkers and has been intensively investigated as a target for imaging and antiangiogenic therapy. Integrin α_v_β_3_ is minimally expressed in normal blood vessels but is significantly overexpressed in newly sprouting vasculature in tumors (4, 5). For targeting purposes, small peptides have been widely used, and the representative peptides include arginine-glycine-aspartic acid (RGD), asparagine-glycine-arginine, histidine-glycine-phenylalanine, and arginine-arginine-leucine (3). The RGD tripeptide sequence is an adhesive protein recognition site, presenting in the extracellular matrix and blood. Integrin α_v_β_3_ binds extracellular matrix proteins through the exposed RGD tripeptide sequence. Although both linear and cyclic RGD peptides have been proven to be valuable in imaging tumor neovasculature, the cyclic form appears superior to the linear form in the aspect of pharmacokinetics because cyclic peptides are trapped in the active conformation and thus are more resistant to proteolysis in vivo (6). To optimize the pharmacokinetic behavior of RGD peptides, the peptides have been further modified with the introduction of sugar moieties or by coupling with a chelating agent or polyethylene glycol. In general, RGD peptides are less selective (binding with 8 of the 24 integrins), degrade rapidly in vivo, and have a relatively low binding affinity (3, 7). Beside peptides, several classes of peptidomimetic antagonists have also been synthesized, which consist of a rigid core scaffold bearing basic and acidic groups that mimic the guanidine and carboxylate groups of the RGD sequence (8). Peptidomimetic antagonist-conjugated magnetic nanoparticles have been demonstrated to delineate very small regions (~30 mm^3^) of angiogenesis and enable phenotyping and staging of early tumors in a clinical setting. Improving the binding affinity and increasing the circulation time of peptides are still the key topics for successful imaging of angiogenesis.

Bunschoten et al. synthesized ^111^In-MSAP-RGD by modifying the cyclic RGD peptides with DTPA and labeling them with a Cy5.5 derivative (CyAL-5.5b) and ^111^In (1). This agent was tested for its effectiveness for imaging tumors, identifying lymph node metastasis, and visualizing tumor margins for surgery (1). This chapter summarizes the data obtained with ^111^In-MSAP-RGD.

### Related Resource Links:

Integrin α_v_β_3_-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Integrin%20%CE%B1v%CE%B23%20%20AND%20micad%5bbook%5d)

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Articles on integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim/?term=integrin) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrials.gov

Reference sequences of integrin members (http://www.ncbi.nlm.nih.gov/gene?term=integrin) in RefSeq

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22505018)]

The RGD peptide c[RGDfK] was synthesized with solid-phase peptide synthesis (1). MSAP, which contains CyAL-5.5b and DTPA, was synthesized as described elsewhere (9). c[RGDfK] was then conjugated with MSAP by overnight reaction at room temperature. After purification, the yield of MSAP-RGD was 84% with a molecular weight of 2,172.9. DTPA-RGD was also synthesized by reaction of DTPA with c[RGDfK]. The yield of DTPA-RGD was 36%, with a molecular weight of 978.7. There was no detailed description regarding the relative amount of each component in the final product.

MSAP-RGD and DTPA-RGD were radiolabeled with ^111^InCl_3_ by 30 min incubation (1). The labeling was confirmed with thin-layer chromatography. The labeling efficacy was reported to be >99% in all cases. The radiochemical yield, specific activity, and radiochemical purity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22505018)]

The cell-binding capability of MSAP-RGD was evaluated with cultured MDAMB231^CXCR4+^ (no expression of α_v_β_3_) and GEβ3 cells (increased α_v_β_3_ expression) and validated with phycoerythrin-labeled monoclonal anti-integrin β_3_ antibody (1). Cells were incubated with the agent for 1 h at 4°C, and flow cytometry showed that MSAP-RGD bound to the α_v_β_3_ integrin-expressing GEβ3 cells, yielding a pattern similar to that of the labeling with the antibody. The mean fluorescence intensity ratio (MFIR) was calculated by dividing the mean fluorescence signal from incubated cells by the background fluorescence signal from cells that were not incubated. The MFIR was 17.1 and 4.1 for the antibody and the MSAP-RGD, respectively. However, MSAP-RGD also exhibited some nonspecific binding with the MDAMB231 cells. These results indicated that RGD in the MSAP-RGD conjugate retained its binding affinity for α_v_β_3_ integrin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22505018)]

Bunschoten et al. tested the effectiveness of ^111^In-MSAP-RGD for imaging tumors in animal models and compared this with data obtained with ^111^In-DTPA-RGD (1). The tumor animal model was developed by transplanting 4T1-luc+ tumor cells into the fourth mammary fat pad of Balb/c nude mice. Single-photon emission computed tomography/computed tomography (SPECT/CT) imaging was performed at 24 h after intravenous injection of ^111^In-MSAP-RGD (40 mg (18 nmol, 10 MBq (0.27 mCi))) or ^111^In-DTPA-RGD (25 mg (25 nmol, 10 MBq (0.27 mCi))) (n = 5 mice/agent). After the SPECT imaging, fluorescent imaging was performed before and after dissecting the organs. The fluorescent signal intensity and radioactivity in organs were quantified. The distribution data showed that both ^111^In-MSAP-RGD and ^111^In-DTPA-RGD accumulated significantly in the tumors relative to other organs (Table 1). Although the relative distribution of the two imaging agents was approximately the same, the background signals (percentage of the injected dose per gram tissue (% ID/g)) obtained with ^111^In-MSAP-RGD were, on average, higher by a factor 10 at 24 h after injection. However, the tumor/muscle ratios for the ^111^In-MSAP-RGD (9.03 ± 3.81) and ^111^In-DTPA-RGD (11.11 ± 4.16) were almost identical. Blocking studies were not performed.

Bunschoten et al. hypothesized that the increased retention of ^111^In-MSAP-RGD might be due to the interactions of the fluorescent dye with albumin; therefore, the biodistribution of albumin was determined by injection (the exact dose was not reported) of ^99m^Tc-vasculosis (^99m^Tc-labeled albumin) (n = 3 mice) (1). At 24 h after injection, the ratio of ^99m^Tc-vasculosis/^111^In-MSAP-RGD was 1.4 ± 0.8 (average of all measured organs excluding tumor and blood; a ratio of 1 would mean complete overlap), whereas the ratio of ^99m^Tc-vasculosis/^111^In-DTPA-RGD was 16.2 ± 10.2. This similarity in distribution between ^99m^Tc-vasculosis and ^111^In-MSAP-RGD indicated the involvement of albumin in the distribution of ^111^In-MSAP-RGD.

Confocal and fluorescent microscopy confirmed the presence of ^111^In-MSAP-RGD in the excised tumors. ^111^In-MSAP-RGD could also be visualized with ex vivo fluorescence imaging of the organs, showing strong signals from the primary tumor, metastases, kidneys, and liver. No or very low fluorescence was observed from the (coagulated) blood, brain, heart, lungs, spleen, muscle, mammary fat pad, and lymph nodes. Because the tumor rim had the highest blood vessel density, the rim contained significant amounts of the RGD probe. Fluorescence imaging outlined the tumor margins, which is required for the surgical removal of tumor tissue. The high vascularization in the peripheral area of tumors was confirmed with FITC-lectin perfusion experiments and CD31 fluorescence immunohistochemistry. Because of the tissue attenuation of the fluorescent signal, the metastases could not initially be detected with fluorescence imaging alone. Guided by the preoperative SPECT/CT image, however, it was possible to locate the metastases through fluorescence imaging after removal of overlying tissues.

Table 1: Biodistribution of ^111^In-DTPA-RGD, ^111^In-MSAP-RGD, and ^99m^Tc-HSA (% ID/g).

Organ | ^111^In-DTPA-RGD | ^111^In-MSAP-RGD | Ratio* | ^99m^Tc-HSA
Blood | 0.03 ± 0.01 | 0.13 ± 0.02 | 5.2 | 3.74 ± 0.21
Brain | 0.02 ± 0.03 | 0.05 ± 0.01 | 2.1 | 0.10 ± 0.01
Lungs | 0.07 ± 0.02 | 1.00 ± 0.29 | 14.0 | 1.80 ± 0.43
Heart | 0.03 ± 0.01 | 0.70 ± 0.12 | 22.6 | 1.31 ± 0.24
Liver | 0.27 ± 0.10 | 4.87 ± 1.17 | 17.9 | 1.98 ± 0.16
Kidneys | 0.78 ±0.10 | 9.26 ± 1.40 | 11.8 | 3.83 ± 0.25
Spleen | 0.17 ± 0.08 | 1.61 ± 0.60 | 10.6 | 1.52 ± 0.16
Stomach | 0.07 ± 0.02 | 0.69 ± 0.21 | 10.4 | 0.81 ± 0.13
Intestines | 0.09 ± 0.02 | 0.98 ± 0.24 | 11.1 | 1.83 ± 0.12
Muscle (paw) | 0.03 ± 0.01 | 0.31 ± 0.08 | 12.1 | 0.27 ± 0.13
Fat (neck) | 0.02 ± 0.01 | 0.28 ± 0.12 | 11.1 | 0.48 ± 0.04
Mammary gland | 0.03 ± 0.01 | 0.25 ± 0.10 | 8.3 | 0.68 ± 0.40
Inguinal LN* | 0.04 ± 0.02 | 0.42 ± 0.27 | 11.7 | 0.81 ± 0.22
Axillary LN* | 0.12 ± 0.06 | 0.98 ± 0.33 | 8.5 | 1.86 ± 0.26
Tumor | 0.26 ± 0.03 | 2.59 ± 0.55 | 10.0 | n.d.
Tumor/Muscle | 11.11 ± 4.16 | 9.03 ± 3.81

*Ratio = ^111^In-MSAP-RGD/^111^In-DTPA-RGD; LN = lymph node.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Bunschoten A., Buckle T., Visser N.L., Kuil J., Yuan H., Josephson L., Vahrmeijer A.L., van Leeuwen F.W. (2012). Multimodal interventional molecular imaging of tumor margins and distant metastases by targeting alphavbeta3 integrin. Chembiochem.
2 Cai W. (2008). andChen, X. Multimodality molecular imaging of tumor angiogenesis. J Nucl Med.
3 Lu X. (2012). andWang, R.F. A concise review of current radiopharmaceuticals in tumor angiogenesis imaging. Curr Pharm Des.
4 Beer A.J. (2008). andSchwaiger, M. Imaging of integrin alphavbeta3 expression. Cancer Metastasis Rev.
5 Gaertner, F.C.,Schwaiger, M., and Beer, A.J. Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging. 2010
6 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
7 Turkbey B., Kobayashi H., Ogawa M., Bernardo M., Choyke P.L. (2009). Imaging of tumor angiogenesis: functional or targeted?. AJR Am J Roentgenol.
8 Jang B.S., Lim E., Hee Park S., Shin I.S., Danthi S.N., Hwang I.S., Le N., Yu S., Xie J., Li K.C., Carrasquillo J.A., Paik C.H. (2007). Radiolabeled high affinity peptidomimetic antagonist selectively targets alpha(v)beta(3) receptor-positive tumor in mice. Nucl Med Biol.
9 Shao F., Yuan H., Josephson L., Weissleder R., Hilderbrand S.A. (2011). Facile Synthesis of Monofunctional Pentamethine Carbocyanine Fluorophores. Dyes Pigm.